# [2[[2-[[[3-(4-chlorophenyl)-8-methyl-8-azabicyclo[3,2,1]-oct-2-yl]-methyl](2-mercaptoethyl)amino]ethyl]amino]ethanethiolato(3-)-N2,N2’,S2,S2]oxo-[1R-exo-exo)])- [^99m^Tc]-technetium

Chemical name: | [2[[2-[[[3-(4-chlorophenyl)-8-methyl-8-azabicyclo[3,2,1]-oct-2-yl]-methyl](2-mercaptoethyl)amino]ethyl]amino]ethanethiolato(3-)-N2,N2’,S2,S2]oxo-[1R-exo-exo)])- [^99m^Tc]-technetium
Abbreviated name: | ^99m^Tc-TRODAT-1
Synonym: | ^99m^Tc-NC100697
Agent Category: | Compound
Target: | Dopamine transporters
Target Category: | Binding
Method of detection: | SPECT
Source of signal: | ^99m^Tc
Activation: | Not required
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-TRODAT-1)]

Dopamine is a neurotransmitter that modulates a variety of human functions such as motion, cognition, emotions, and the peristaltic reflexes in the gastrointestinal tract. The transport of this molecule at the neuron pre- and postsynaptic junctions is mediated by an axonal membrane dopamine transporter (DAT) that regulates dopamine levels within the synaptic cleft (1). The process of dopamine release and reuptake within the synaptic cleft facilitates nerve transmission. The striatum region of the brain has a high density of DAT and is rich in dopamine. Psychotic drugs such as cocaine, amphetamines, and methylphenidate (MPH) target DAT, which suggests that the dopamine system modulates the mood of an individual (1-3). Also, changes in DAT are of particular interest in individuals with Parkinson’s disease (PD), which is caused by the loss of neurons bearing these transporters in the basal ganglia and substantia nigra regions of the striatum (4). Development of various imaging ligands that specifically bind to DAT has been of interest to understand the functioning of these transporters and also to diagnose and monitor the treatment of PD. Dopamine receptors and transporters have also been suggested to play a role in the development of the heritable and disruptive attention deficit hyperactivity disorder (ADHD) that is sometimes observed in children (5). Although several ligands are available that can be used for DAT imaging, they have a limited availability and require cyclotron-produced radionuclides that have short half-lives (6). In addition, these ligands require from a few hours to >18 hours to reach a suitable concentration at the imaging target area (4).

In an effort to alleviate the limitations observed with the cyclotron-produced radionuclides, DAT ligands labeled with ^99m^Tc were developed for research and possibly for clinical use. These ligands are neutral lipophilic complexes that contain N-(alkylthiolate)tropane, aminobis(ethylthiolate), and a center core of ^99m^Tc (4). The cocaine derivative [2[[2-[[[3-(4-chlorophenyl)-8-methyl-8-azabicyclo[3,2,1]-oct-2-yl]-methyl](2-mercaptoethyl)amino]ethyl]amino]ethanethiolato(3-)-N2,N2’,S2,S2]oxo-[1R-exo-exo)])- [^99m^Tc]-technetium (^99m^Tc-TRODAT-1) is a ligand that belongs to this group. Hu et al. suggested the possible benefit of ^99m^Tc-TRODAT-1 for an early and differential diagnosis of PD (7).

The application of ^99m^Tc-TRODAT-1 for the imaging of DAT is reviewed in this chapter.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-TRODAT-1%20synthesis)]

The synthesis of ^99m^Tc-TRODAT-1 has been described by Meegalla et al. (4). Due to the complex intermediate compounds synthesized to obtain ^99m^Tc-TRODAT-1, only general terms have been used in this chapter. The reader should refer to the original publication for complete names (4).

Briefly, the synthesis of a 3β-(p-chloro-)tropane ester and the corresponding carboxylic acid was performed as detailed elsewhere (8, 9). A corresponding acyl chloride was obtained by the action of oxalyl chloride on the carboxylic acid at room temperature. This compound was treated with an amine to obtain the corresponding amide. A secondary amine was prepared by diborane reduction of the amide and converted to a tertiary amide by alkylation with alkyl chloride. The amide functions of compound 9 were reduced with BH_3_•THF to obtain the amine compound 11a. TRODAT-1 was obtained by deprotection of compound 11a with Hg(OAc)_2_.

To radiolabel with ^99m^Tc, TRODAT-1 was dissolved in ethanol and HCl, and a Sn-glucoheptonate solution containing EDTA was successively added to it. Subsequently, a saline solution containing ^99m^Tc-pertechnetate was added to the mixture, which was then heated to 100^o^C for 30 min. The mixture was then cooled to room temperature and neutralized with a saturated solution of NaHCO_3_. The ^99m^Tc-TRODAT-1 complex was extracted from the aqueous solution with ethyl acetate, passed through a column of Na_2_SO_4_, and the ethyl acetate was removed under a flow of nitrogen. The resultant residue was dissolved in ethanol and purified by high-performance liquid chromatography. The radiochemical yield of the reaction was 88% with a radiochemical purity of 98%. The specific activity of the radiolabeled compound was not provided in the publication.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc%20TRODAT-1%20in%20vitro)]

The affinity constant (K_i_) of ^99m^Tc-TRODAT-1 in rat brain sections was determined using the surrogate molecule rhenium-TRODAT-1 (Re-TRODAT-1) to be 14.1 nM (10). In another study with rat tissue homogenates, the K_i_ of ^99m^Tc-TRODAT-1 for DAT and the serotonin transporter was determined using Re-TRODAT-1 to be 14.1 ± 2.1 and 360 ± 44 nM, respectively (11).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-TRODAT-1+rodentia&WebEnv=0T3yIn6j5P6oAztD3kIUQhM5Y8MDj9SZE9_rnMM94WwXjaSaSTAm5u8sjK-Ccf-W-_YKhvzA3AFA62%40D4761739635E72B0_0076SID&WebEnvRq=1)]

Hwang et al. investigated the effect of DAT competitors 1-methyl-4-phenyl-1,2,3,6-tetrahydropyridine (MPTP), levadopa (L-DOPA), N-methyl-2β-carbomethoxy-3β-(4fluorophenyl)tropane (CFT, WIN 35,428), and MPH on the biodistribution of ^99m^Tc-TRODAT-1 in mice (12). Compared to controls, mice treated with MPTP and L-DOPA did not show significant differences in radiolabel uptake in bilateral striata of the brain. Almost no ^99m^Tc-TRODAT-1 binding was observed in mice treated with CFT or MPH. The investigators concluded that ^99m^Tc-TRODAT-1 could probably be used for clinical investigation of neurological disorders such as PD.

Acton et al. used ^99m^Tc-TRODAT-1 to demonstrate that DAT binding could be quantified and studied accurately in mice with ultrahigh-resolution single-photon emission computed tomography (SPECT) (13). Similarly, Chen et al. demonstrated that ^99m^Tc-TRODAT-1 could be used to study DAT in a rodent model that used rats treated with 6-hydroxydopamine (14). Fang et al. showed that ^99m^Tc-TRODAT-1 was a safe and useful imaging agent to investigate localization of presynaptic DAT in rodent brain (15). Dresel et al. showed that ^99m^Tc-TRODAT-1 binding in rats was affected only if the animals were pretreated with drugs that significantly increased dopamine levels or competed with DAT binding (16). The investigators suggested that prior knowledge of drugs being administered to patients could help interpret DAT status in individuals being evaluated by SPECT with ^99m^Tc-TRODAT-1 in a clinical setting.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-TRODAT-1+non-primate+mammals&WebEnv=0XLx3dpxs0qff4VrwiKceM58aSHDWGkMf93mDz6ei_m4yUV3fsdnLVqsf25Ha7_tZyj3HennKc8E8D%40D4761739635E72B0_0076SID&WebEnvRq=1)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-TRODAT-1+nonhuman+primates&WebEnv=0nYNgSUnnXZKN1QJUrN1A9soxGnXbk7gysXqtvAqXGEC9Yi9nGbA6WLm-66vJ0gi5QFhM79LTQoZAM%40D4761739635E72B0_0076SID&WebEnvRq=1)]

In an effort to study the pre- and postsynaptic dopamine systems in a primate model, the technique of dual SPECT with ^99m^Tc-TRODAT-1 and ^123^I-labeled iodobenzamide was used with baboons (17) and Formosan rock monkeys (18). From these studies it was concluded that the use of a dual-isotope technique could be an effective method to gain a better insight into the dopaminergic system. In another study, the uptake ratio of ^99m^Tc-TRODAT-1 in the striatum versus the cerebellum of normal and hemi-Parkinsonian monkeys was determined (7). The investigators demonstrated that the striatum/cerebellum ratio of ^99m^Tc-TRODAT-1 uptake in the hemi-Parkinsonian animals was significantly lower compared to that of controls.

Xiao et al investigated the effect of an acute morphine injection on the functional changes of DAT in rhesus monkeys (19). A rapid downregulation of DAT in the morphine-treated monkeys was observed, and this was only partially reversible with cessation of morphine. The investigators suggested that the striatum is an effective target of morphine and that DAT function could be used as an indicator of morphine addiction.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-TRODAT-1+humans&WebEnv=0ROLqMmFJnRHngpgvwr4whNNwVyICAw1vnXBoNIlD3mfbIhRGZK_1y_2l3wnEukQIixKJN3IV1Y1Ap%40D4761739635E72B0_0076SID&WebEnvRq=1)]

^99m^Tc-TRODAT-1 scintigraphy was shown to have a high sensitivity and specificity to measure the gradual loss of DAT in PD patients (20). The investigators suggested the use of this radiolabeled compound for the possible diagnosis of PD. In another study, the possible use of SPECT with ^99m^Tc-TRODAT-1 to distinguish between PD and essential tremor was suggested (21).

The distribution volume ratios (DVRs) of ^99m^Tc-TRODAT-1 binding affinity was determined from SPECT data for patients with low and high depressive symptoms (22). Data obtained from this study suggested that the ^99m^Tc-TRODAT-1 binding affinity to DAT may be associated with the depressive effect. The study also supported an earlier study (23) that showed an elevated ^99m^Tc-TRODAT-1 DVR in patients in a high depressive state. In a pilot study designed to investigate the effect of estrogen replacement therapy (ERT) on DAT availability in the brains of healthy postmenopausal women, an increase in DAT in the putamen region of the brain was observed (24). This indicated a possible association of ERT with improvement in PD and late-onset schizophrenia.

The possible role of the degree of ^99m^Tc-TRODAT-1 binding to striatal DAT and the response to MPH in patients with attention deficit hyperactivity disorder (ADHD) was investigated (25). Data from the study showed that individuals with ADHD who have an elevated striatal DAT responded better to MPH therapy than those with low DAT levels. On the basis of these results, the possible use of DAT measurements to predict a response to MPH therapy was suggested. In another study that used ^99m^Tc-TRODAT-1, it was shown that the decrease in the number of DAT binding sites in ADHD patients receiving MPH therapy correlated with an improvement in clinical symptoms (26).

A new formulation of ^99m^Tc-TRODAT-1 was evaluated in a phase-I human clinical trial to characterize striatal DAT binding and to determine if the physiological age and sex of trial participants had an effect on binding (6). The investigators observed an age- and sex-dependency (especially in postmenopausal women) for the binding of this radionuclide. On the basis of this data, the investigators suggested that the age and sex of individuals being studied with ^99m^Tc-TRODAT-1 should be taken into consideration while data after scintigraphy is evaluated.

## Supplemental Information

[Disclaimers]

Toxicology

Pharmacology

Dosimetry

## NIH Support

Parts of the studies presented in this chapter were funded by NIH grant #s AG-17524, DA-09469, NS24538 and NS18509.

## References

1 Amara S.G., Kuhar M.J. (1993). Neurotransmitter transporters: recent progress. Annu Rev Neurosci.
2 Goeders N.E., Smith J.E. (1983). Cortical dopaminergic involvement in cocaine reinforcement. Science.
3 Volkow N.D., Wang G.J., Fowler J.S., Gatley S.J., Ding Y.S., Logan J., Dewey S.L., Hitzemann R., Lieberman J. (1996). Relationship between psychostimulant-induced "high" and dopamine transporter occupancy. Proc Natl Acad Sci U S A.
4 Meegalla S.K., Plossl K., Kung M.P., Chumpradit S., Stevenson D.A., Kushner S.A., McElgin W.T., Mozley P.D., Kung H.F. (1997). Synthesis and characterization of technetium-99m-labeled tropanes as dopamine transporter-imaging agents. J Med Chem.
5. Thapar, A., M. O'Donovan, and M.J. Owen, The genetics of attention deficit hyperactivity disorder. Hum Mol Genet, 2005. 14 Spec No. 2: p. R275-82.
6 Koch W., Pogarell O., Popperl G., Hornung J., Hamann C., Gildehaus F.J., Seelos K., Lewis D., Favit A., Tatsch K. (2007). Extended studies of the striatal uptake of 99mTc-NC100697 in healthy volunteers. J Nucl Med.
7 Hu P., Chen L., Zhang H.Q., Li J.R., Liang H. (2004). Single photon emission computer tomography of dopamine transporters in monkeys and humans with 99mTc-TRODAT-1. Chin Med J (Engl).
8 Carroll F.I., Abraham P., Lewin A.H., Parham K.A., Boja J.W., Kuhar M. (1992). Isopropyl and phenyl esters of 3 beta-(4-substituted phenyl)tropan-2 beta-carboxylic acids. Potent and selective compounds for the dopamine transporter. J Med Chem.
9 Meltzer P.C., Liang A.Y., Brownell A.L., Elmaleh D.R., Madras B.K. (1993). Substituted 3-phenyltropane analogs of cocaine: synthesis, inhibition of binding at cocaine recognition sites, and positron emission tomography imaging. J Med Chem.
10 Kung M.P., Stevenson D.A., Plossl K., Meegalla S.K., Beckwith A., Essman W.D., Mu M., Lucki I., Kung H.F. (1997). [99mTc]TRODAT-1: a novel technetium-99m complex as a dopamine transporter imaging agent. Eur J Nucl Med.
11 Dresel S.H., Kung M.P., Huang X., Plossl K., Hou C., Shiue C.Y., Karp J., Kung H.F. (1999). In vivo imaging of serotonin transporters with [99mTc]TRODAT-1 in nonhuman primates. Eur J Nucl Med.
12 Hwang J.J., Liao M.H., Yen T.C., Wey S.P., Lin K.J., Pan W.H., Chen J.C., Ting G. (2002). Biodistribution study of [99mTc] TRODAT-1 alone or combined with other dopaminergic drugs in mice with macroautoradiography. Appl Radiat Isot.
13 Acton P.D., Choi S.R., Plossl K., Kung H.F. (2002). Quantification of dopamine transporters in the mouse brain using ultra-high resolution single-photon emission tomography. Eur J Nucl Med Mol Imaging.
14 Chen Y.K., Liu R.S., Huang W.S., Wey S.P., Ting G., Liu J.C., Shen Y.Y., Wan F.J. (2001). The role of dopamine transporter imaging agent [99mTc]TRODAT-1 in hemi-parkinsonism rat brain. Nucl Med Biol.
15 Fang P., Wu C.Y., Liu Z.G., Wan W.X., Wang T.S., Chen S.D., Chen Z.P., Zhou X. (2000). The preclinical pharmacologic study of dopamine transporter imaging agent [99mTc]TRODAT-1. Nucl Med Biol.
16 Dresel S.H., Kung M.P., Plossl K., Meegalla S.K., Kung H.F. (1998). Pharmacological effects of dopaminergic drugs on in vivo binding of [99mTc]TRODAT-1 to the central dopamine transporters in rats. Eur J Nucl Med.
17 Dresel S.H., Kung M.P., Huang X.F., Plossl K., Hou C., Meegalla S.K., Patselas G., Mu M., Saffer J.R., Kung H.F. (1999). Simultaneous SPECT studies of pre- and postsynaptic dopamine binding sites in baboons. J Nucl Med.
18 Ma K.H., Huang W.S., Chen C.H., Lin S.Z., Wey S.P., Ting G., Wang S.D., Liu H.W., Liu J.C. (2002). Dual SPECT of dopamine system using [99mTc]TRODAT-1 and [123I]IBZM in normal and 6-OHDA-lesioned formosan rock monkeys. Nucl Med Biol.
19 Xiao Z.W., Cao C.Y., Wang Z.X., Li J.X., Liao H.Y., Zhang X.X. (2006). Changes of dopamine transporter function in striatum during acute morphine addiction and its abstinence in rhesus monkey. Chin Med J (Engl).
20 Weng Y.H., Yen T.C., Chen M.C., Kao P.F., Tzen K.Y., Chen R.S., Wey S.P., Ting G., Lu C.S. (2004). Sensitivity and specificity of 99mTc-TRODAT-1 SPECT imaging in differentiating patients with idiopathic Parkinson's disease from healthy subjects. J Nucl Med.
21 Wang J., Jiang Y.P., Liu X.D., Chen Z.P., Yang L.Q., Liu C.J., Xiang J.D., Su H.L. (2005). 99mTc-TRODAT-1 SPECT study in early Parkinson's disease and essential tremor. Acta Neurol Scand.
22 Newberg A., Amsterdam J., Shults J. (2007). Dopamine transporter density may be associated with the depressed affect in healthy subjects. Nucl Med Commun.
23 Brunswick D.J., Amsterdam J.D., Mozley P.D., Newberg A. (2003). Greater availability of brain dopamine transporters in major depression shown by [99m Tc]TRODAT-1 SPECT imaging. Am J Psychiatry.
24 Gardiner S.A., Morrison M.F., Mozley P.D., Mozley L.H., Brensinger C., Bilker W., Newberg A., Battistini M. (2004). Pilot study on the effect of estrogen replacement therapy on brain dopamine transporter availability in healthy, postmenopausal women. Am J Geriatr Psychiatry.
25 la Fougere C., Krause J., Krause K.H., Josef Gildehaus F., Hacker M., Koch W., Hahn K., Tatsch K., Dresel S. (2006). Value of 99mTc-TRODAT-1 SPECT to predict clinical response to methylphenidate treatment in adults with attention deficit hyperactivity disorder. Nucl Med Commun.
26 Dresel S., Krause J., Krause K.H., LaFougere C., Brinkbaumer K., Kung H.F., Hahn K., Tatsch K. (2000). Attention deficit hyperactivity disorder: binding of [99mTc]TRODAT-1 to the dopamine transporter before and after methylphenidate treatment. Eur J Nucl Med.